# Quantum dots-deoxycholic acid (DOCA)-conjugated low molecular weight heparin (LMWH) nanoparticles

Chemical name: | Quantum dots-deoxycholic acid (DOCA)-conjugated low molecular weight heparin (LMWH) nanoparticles
Abbreviated name: | Q-LHD, Q-LHD5
Synonym:
Agent category: | Compound
Target: | Bile acid transporter
Target category: | Transporter
Method of detection: | Optical, near-infrared fluorescence (NIR)
Source of signal: | Quantum dot (QD)
Activation: | No
Studies: | - In vitro; - Rodents | Structure is not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Q-LHD)]

Optical fluorescence imaging is increasingly used to monitor biological functions of specific targets in small animals (1-3). However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light (350–650 nm) are used. Near-infrared (NIR) fluorescence (650–1,000 nm) detection avoids the background fluorescence interference of natural biomolecules, providing a high contrast between target and background tissues. NIR fluorophores have wider dynamic range and minimal background as a result of reduced scattering compared with visible fluorescence detection. They also have high sensitivity, resulting from low infrared background, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is becoming a noninvasive complement to radionuclide imaging in small animals (4, 5).

Fluorescent semiconductor quantum dots (QDs) are nanocrystals made of CdSe/CdTe/ZnS with radii of 1–10 nm (6-8). They can be tuned to emit fluorescence signals in a range of wavelengths by changing their sizes and composition, thus providing broad excitation profiles and high absorption coefficients. They have narrow, symmetric emission spectra with long, excited-state lifetimes (20–50 ns) compared to those of fluorescent dyes (1–10 ns). They possess good quantum yields of 40%–90% and high extinction coefficients. QDs are more photo-stable than conventional organic dyes. They can be coated and capped with hydrophilic materials for additional conjugation with biomolecules, such as peptides, antibodies, nucleic acids, and small organic compounds, which have been tested in vitro and in vivo (8-12). Although many cells have been labeled with QDs in vitro with little cytotoxicity, there are limited studies of long-term toxicity of QDs in small animals (13-21). Little is known about the toxicity and the mechanisms of clearance and metabolism of QDs in humans.

Low molecular weight heparin (LMWH) is a glycosaminoglycan that is widely used as an anticoagulant agent (22). LMWH was reported to inhibit cancer progression through its anti-angiogenic and anti-metastatic effects (23). However, LMWH has to be injected intravenously due to its poor absorption in the intestines. Deoxycholic acid (DOCA)-conjugated LMWH (LHD) was found to be absorbed in the small intestine via the bile acid transporter after oral administration to rodents and monkeys (24). Khatun et al. (25, 26) prepared LHD micelles loaded with NIR fluorescence QDs (Q-LHD nanoparticles) as an oral imaging agent for optical imaging of the small intestines.

### Related Resource Links:

- Chapters in MICAD (QDs (http://www.ncbi.nlm.nih.gov/books?term=Quantum%20dot%5BAll%20Fields%5D%20AND%20micad%5Bbook%5D), heparin (http://www.ncbi.nlm.nih.gov/books?term=heparin%5BAll%20Fields%5D%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (bile acid transporter (http://www.ncbi.nlm.nih.gov/gene/6555))
- Articles in Online Mendelian Inheritance in Man (OMIM) (bile acid transporter (http://omim.org/entry/601295))
- Clinical trials (heparin (http://www.clinicaltrials.gov/ct2/results?term=heparin&Search=Search))
- Drug information in FDA (heparin (http://google2.fda.gov/search?q=heparin&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&filter=1))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Q-LHD%20and%20synthesis)]

LHD was prepared by conjugation of the hydroxyl group of DOCA with the carboxylic group of LMWH (26). DOCA was aminated by reaction with 4-methylmorpholine and ethylenediamine overnight at room temperature. An aqueous solution of LMWH (pH 5) was added to a solution of the aminated DOCA, 1-ethyl-3-(3-dimethylaminopropyl)-carbodiimide and N-hydroxysuccinimide. After incubation for 30 min, LHD (diameter = 187 ± 32 nm) was purified with dialysis, with 44% yield and 82% purity. There were five DOCA moieties per LMWH. QDs (CdSe/CdTe) (56 nmol Cd, 7 nm in diameter) with an emission maximum at 675 nm were mixed with 50 mg LHD in chloroform for 18 h. After evaporation of the organic solvent, the mixture was dialyzed for 48 h with an aqueous solution. Q-LHD nanoparticles were isolated with filtration, with 81% yield. Q-LHD nanoparticles had a diameter of 220 ± 26 nm as measured with electrophoretic light scattering (ELS). The zeta potential values were −68, 25, and −7.3 mV for LHD, QD, and Q-LHD, respectively. The diameters of LHD and Q-LHD nanoparticles remained similar after incubation in phosphate-buffered saline (PBS) for 2 h at pH 5, 7, and 9 as measured with ELS. The diameter and fluorescence intensity of Q-LHD remained little changed after 5 d incubation in 10% fetal bovine serum.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Q-LHD%20and%20in%20vitro)]

Khatun et al. (26) showed that there was little release of QDs from Q-LHD for up to 5 d (room temperature) at pH 7.4 and pH 9. On the other hand, the release of QDs was higher at pH 1.5 and pH 5 compared with pH 7.4 and pH 9. In vitro cytotoxicity and cellular uptake assays were performed by incubation of Caco-2 cells with different concentrations of Q-LHD (0.1–100 µg/mL) for 24 h and 48 h at 37ºC. Cell viability was 80%–95% at 24 h and 60%–70% at 48 h. Confocal laser scanning microscopy showed the presence of Q-LHD on the cell surface and inside the cell membrane after 1 h at 37ºC.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Q-LHD%20and%20rodentia)]

Khatun et al. (26) performed NIR fluorescence imaging studies with female nude mice (n = 4/group) at 2–36 h after oral administration of 2.5 mg/kg and 5.0 mg/kg Q-LHD. Whole-body small animal images were obtained with a time-domain diffuse optical tomography system. The QD signal was found mainly in the stomach at 2 h and was detected in the duodenum, jejunum, and ileum at 8 h. The QD signals were clearly visualized in the lung, heart, liver, spleen, rectum, kidneys, small intestines, and stomach at 8 h. By 24 h, most of the signal intensity from the 2.5 mg/kg dose in the stomach was gone, but the signal from the 5.0 mg/kg dose persisted at this time point. By 36 h, most of the signal intensity was gone from the images. Analysis of the excised tissues at 36 h showed only a negligible amount of Cd^3+^ (<0.0045 µg Cd/g tissue) in the kidney, liver, lung, heart, duodenum, jejunum, and ileum. Oral administration of taurocholic acid (TCA) (0, 25, and 50 mg/kg) 1.5 h before oral administration of 2.5 mg/kg Q-LHD exhibited a dose-dependent inhibition of signal intensity in the small intestines at 8 h. The highest dose of TCA completely inhibited the signal intensity in the intestinal area, suggesting that TCA and DOCA bind to the bile acid transporter in the small intestines.

Khatun et al. (25) performed ex vivo NIR fluorescence imaging studies with female nude mice (n = 3/group) at 8 h after oral administration of 2.5 mg/kg or 5.0 mg/kg Q-LHD. The highest fluorescence intensity was observed in the ileum and was expressed as 100% relative fluorescence units (RFU) with the higher oral dose. The jejunum showed 75% RFU, whereas the duodenum, stomach, liver, heart, and kidney showed <10% RFU. The oral dose of 2.5 mg/kg showed slightly lower RFU than the 5.0 mg/kg dose in the tissues examined. Plasma concentration of Q-LHD was assessed with anti-Factor Xa activity of LMWH. Plasma concentration of oral doses of Q-LHD appeared at 30 min and peaked at 120 min before declining. The maximum plasma concentrations were 0.82 ± 0.19 and 0.95 ± 0.30 IU/mL for 2.5 mg/kg and 5.0 mg/kg Q-LHD, respectively. NIR fluorescence measurements of the plasma followed the time pattern for anti-Factor Xa measurements. Therefore, Q-LHD nanoparticles were rapidly absorbed in the intestines and found in the blood circulation. Transition electron microscopy showed the presence of Q-LHD nanoparticles in the jejunum and ileum, but not in the stomach and duodenum, at 8 h.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Q-LHD%20and%20%28dog%20or%20pig%20or%20rabbit%20or%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Q-LHD%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Q-LHD%20and%20human%20not%20animal%20not%20cell%20line)]

No publication is currently available.

## References

1 Hargreaves R.J. (2008). The role of molecular imaging in drug discovery and development. Clin Pharmacol Ther.
2 Pan D., Caruthers S.D., Chen J., Winter P.M., SenPan A., Schmieder A.H., Wickline S.A., Lanza G.M. (2010). Nanomedicine strategies for molecular targets with MRI and optical imaging. Future Med Chem.
3 Willmann J.K., van Bruggen N., Dinkelborg L.M., Gambhir S.S. (2008). Molecular imaging in drug development. Nat Rev Drug Discov.
4 Tung C.H. (2004). Fluorescent peptide probes for in vivo diagnostic imaging. Biopolymers.
5 Leung K., Chopra A., Shan L., Eckelman W.C., Menkens A.E. (2012). Essential parameters to consider for the characterization of optical imaging probes. Nanomedicine (Lond).
6 Chan W.C., Maxwell D.J., Gao X., Bailey R.E., Han M., Nie S. (2002). Luminescent quantum dots for multiplexed biological detection and imaging. Curr Opin Biotechnol.
7 Gao X., Yang L., Petros J.A., Marshall F.F., Simons J.W., Nie S. (2005). In vivo molecular and cellular imaging with quantum dots. Curr Opin Biotechnol.
8 Michalet X., Pinaud F.F., Bentolila L.A., Tsay J.M., Doose S., Li J.J., Sundaresan G., Wu A.M., Gambhir S.S., Weiss S. (2005). Quantum dots for live cells, in vivo imaging, and diagnostics. Science.
9 Alivisatos A.P., Gu W., Larabell C. (2005). Quantum dots as cellular probes. Annu Rev Biomed Eng.
10 Hilger I., Leistner Y., Berndt A., Fritsche C., Haas K.M., Kosmehl H., Kaiser W.A. (2004). Near-infrared fluorescence imaging of HER-2 protein over-expression in tumour cells. Eur Radiol.
11 Medintz I.L., Uyeda H.T., Goldman E.R., Mattoussi H. (2005). Quantum dot bioconjugates for imaging, labelling and sensing. Nat Mater.
12 Smith A.M., Gao X., Nie S. (2004). Quantum dot nanocrystals for in vivo molecular and cellular imaging. Photochem Photobiol.
13 Akerman M.E., Chan W.C., Laakkonen P., Bhatia S.N., Ruoslahti E. (2002). Nanocrystal targeting in vivo. Proc Natl Acad Sci U S A.
14 Braydich-Stolle L., Hussain S., Schlager J.J., Hofmann M.C. (2005). In vitro cytotoxicity of nanoparticles in mammalian germline stem cells. Toxicol Sci.
15 Frangioni J.V., Hajjar R.J. (2004). In vivo tracking of stem cells for clinical trials in cardiovascular disease. Circulation.
16 Gao X., Cui Y., Levenson R.M., Chung L.W., Nie S. (2004). In vivo cancer targeting and imaging with semiconductor quantum dots. Nat Biotechnol.
17 Han M., Gao X., Su J.Z., Nie S. (2001). Quantum-dot-tagged microbeads for multiplexed optical coding of biomolecules. Nat Biotechnol.
18 Lovric J., Bazzi H.S., Cuie Y., Fortin G.R., Winnik F.M., Maysinger D. (2005). Differences in subcellular distribution and toxicity of green and red emitting CdTe quantum dots. J Mol Med.
19 Ohnishi S., Lomnes S.J., Laurence R.G., Gogbashian A., Mariani G., Frangioni J.V. (2005). Organic alternatives to quantum dots for intraoperative near-infrared fluorescent sentinel lymph node mapping. Mol Imaging.
20 Shiohara A., Hoshino A., Hanaki K., Suzuki K., Yamamoto K. (2004). On the cyto-toxicity caused by quantum dots. Microbiol Immunol.
21 Soltesz E.G., Kim S., Laurence R.G., DeGrand A.M., Parungo C.P., Dor D.M., Cohn L.H., Bawendi M.G., Frangioni J.V., Mihaljevic T. (2005). Intraoperative sentinel lymph node mapping of the lung using near-infrared fluorescent quantum dots. Ann Thorac Surg.
22 Chen M.C., Wong H.S., Lin K.J., Chen H.L., Wey S.P., Sonaje K., Lin Y.H., Chu C.Y., Sung H.W. (2009). The characteristics, biodistribution and bioavailability of a chitosan-based nanoparticulate system for the oral delivery of heparin. Biomaterials.
23 Ludwig R.J. (2009). Therapeutic use of heparin beyond anticoagulation. Curr Drug Discov Technol.
24 Park J.W., Jeon O.C., Kim S.K., Al-Hilal T.A., Jin S.J., Moon H.T., Yang V.C., Kim S.Y., Byun Y. (2010). High antiangiogenic and low anticoagulant efficacy of orally active low molecular weight heparin derivatives. J Control Release.
25 Khatun Z., Nurunnabi M., Cho K.J., Lee Y.K. (2012). Imaging of the GI tract by QDs loaded heparin-deoxycholic acid (DOCA) nanoparticles. Carbohydr Polym.
26 Khatun Z., Nurunnabi M., Cho K.J., Lee Y.K. (2012). Oral delivery of near-infrared quantum dot loaded micelles for noninvasive biomedical imaging. ACS Appl Mater Interfaces.